# N-(2-[^11^C],5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide

Chemical name: | N-(2-[^11^C],5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide
Abbreviated name: | [^11^C]DAA1106
Synonym:
Agent Category: | Compound
Target: | Peripheral-type benzodiazepine receptor
Target Category: | Receptor binding
Method of detection: | PET
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106)]

Benzodiazepines, such as diazepam, are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been identified as the central benzodiazepine receptor (CBR) and the peripheral benzodiazepine receptor (PBR). CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBR has been studied in vivo with positron emission tomography (PET) using [^11^C]PK11195, an isoquinoline carboxamide with specific PBR-antagonistic activity. [^11^C]PK11195 is being developed as a PET agent for non-invasive study of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBR in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBR in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor. [^11^C]DAA1106 is being developed as a PET agent for the non-invasive study of microglia and macrophage activation in the brain.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20synthesis)]

In the report by Zhang et al. (10), [^11^C]DAA1106 was synthesized by alkylation of the desmethyl precursor (N-(5-fluoro-2-phenoxyphenyl)-N-(2-hydroxy-5-methoxybenzyl)-acetamide) with ^11^C-labeled methyl iodide in the presence of NaH. Subsequent high-performance liquid chromatography (HPLC) separation gave a radiochemical purity >98% with a total synthesis time of 22 min. The specific activity was 90–156 GBq/μmol (2.5–4.3 Ci/μmol) at end of synthesis (EOS). A reproducible radiochemical yield of 72% (decay-corrected) was reported.

Probst et al. (11) automated the synthesis of [^11^C]DAA1106 using a GE gas-phase synthesis module with high radioactivities of ^11^C-labeled methyl iodide. Radiochemical purities of 99% and specific activities of 100–200 GBq/μmol (2.7–5.4 Ci/μmol) were obtained at EOS. The methylation was performed in the presence of NaOH. The total synthesis time was 34 min from end of bombardment to EOS with radiochemical yields of 71–89% at EOS.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20in%20vitro)]

In vitro binding studies of [^3^H]DAA1106 produced dissociation constant (K_d_) values of 0.12 ± 0.03 and 0.43 ± 0.04 nM for mitochondrial fractions of rat and monkey cerebral cortex, respectively (9). The PBR maximal binding (B_max_) values were 161.03 ± 5.8 and 701 ± 70 fmol/mg protein for mitochondrial fractions of rat and monkey cerebral cortex, respectively. Regional distribution of [^3^H]DAA1106 in mitochondrial fractions of the rat brain revealed that the olfactory bulb has the highest B_max_ (>400 fmol/mg protein), followed by the cerebellum, cerebral cortex, hypothalamus, striatum, hippocampus, and thalamus. This pattern of DAA1106 binding in the brain was later confirmed in rats by in vitro autoradiographic studies using [^11^C]DAA1106 (12).

Venneti et al. (13, 14) showed that [^3^H]DAA1106 exhibited ~5-fold lower K_d_ values compared with [^3^H](R)-PK11195 in normal rat brain tissue, whereas B_max_ values were uniformly lower with [^3^H]DAA1106 compared with [^3^H](R)-PK11195. The relative contributions of astrocytes and microglia to [^3^H]DAA1106 bindings as PBR were assessed by combined immunostaining for astrocytes and activated microglia (CD68) with [^3^H]DAA1106 autoradiography on frozen brain sections obtained from rats with traumatic brain injury. [^3^H]DAA1106 binding co-registered with activated microglia more than astrocytes in the region of the contusion. Minimal [^3^H]DAA1106 binding as well as CD68 staining was observed in cortical regions in the contralateral hemisphere. [^3^H]DAA1106 binding was confirmed to be specific because it was displaced by unlabeled DAA1106 (1 ìM) in adjacent sections in the region of the contusion.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20rodentia)]

Biodistribution studies in normal mice showed high accumulation of radioactivity in the lung (70.8% of injected dose (ID)/g), followed by the heart (16.5% ID/g), kidney (10.0% ID/g), adrenal gland (6.6% ID/g), and brain (3.5% ID/g) at 15 min after injection of [^11^C]DAA1106 (10). Radioactivity of the tracer was low in the liver and blood (2% ID/g). The regional distribution in the mouse brain showed rapid accumulation into all brain regions at 1 min after injection. The highest uptake was in the olfactory bulb (4.2% ID/g), followed by the cerebellum (3.5% ID/g), cerebral cortex (2.3% ID/g), striatum (1.8% ID/g), hippocampus (1.7% ID/g), hypothalamus (1.4% ID/g), and thalamus (1.2% ID/g) at 30 min after injection. Coadiministration of unlabeled DAA1106 decreased the accumulation in all brain regions, with the most significant reduction in the olfactory bulb and cerebellum. Almost all of the radioactivity in the brain was intact [^11^C]DAA1106 at 60 min after injection. The fraction of unchanged [^11^C]DAA1106 in blood samples, as determined by HPLC, was 65% at 5 min, 17% at 30 min, and 6% at 60 min. The major metabolite was found to be the debenzylated compound N-(5-fluoro-2-phenoxyphenyl)acetamide, which showed no binding to PBR or CBR (8). In later experiments, Venneti et al. (13) used PET imaging to find that [^11^C]DAA1106 was effectively displaced by DAA1106 in the lung (92%), heart (80%), and brain (75%).

Maeda et al. (12) reported ex vivo autoradiographic studies of [^11^C]DAA1106 brain binding in normal rats and in rats with focal hippocampus lesions induced by kainic acid. [^11^C]DAA1106 binding was highest in the olfactory bulb, followed by the cerebellum, pons/medulla, frontal cortex, and hippocampus at 30 min after injection. [^11^C]DAA1106 binding was increased in the focal hippocampal lesions by 1-fold (P < 0.05) over the control hippocampus, indicating an increase in PBR binding sites associated with microglia infiltration.

Venneti et al. (13) reported that LPS-lesioned rats exhibited increased brain accumulation of [^11^C]DAA1106 compared with [^11^C](R)-PK11195 as imaged by PET. [^11^C](R)-PK11195 accumulation was effectively blocked by either PK11195 or DAA1106, whereas [^11^C]DAA1106 was effectively blocked by DAA1106 and to a lesser extent by PK11195. [^11^C]DAA1106 showed greater retention than [^11^C](R)-PK11195 at the site of the contusion in rats with traumatic brain injury as assessed by ex vivo autoradiography (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

[^11^C]DAA1106 PET imaging was performed in the abdomen of rabbits (n = 3) with accumulation in the kidney cortex at 60–75 min after injection (11). Injection of DAA1106 at 30 min after [^11^C]DAA1106 injection clearly displaced the radioactivity in the kidney cortex, indicating specific binding. The presence of PBR expression in the kidney cortex was confirmed by immunohistochemistry.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20%28primate%20not%20human%29)]

Using PET, Maeda et al. (12) obtained serial brain scans in one baboon after injections of 90.6 ± 9.3 MBq (2.4 ± 0.3 mCi) of [^11^C]DAA1106. Accumulation of radioactivity in the brain (occipital cortex, frontal cortex, and cerebellum) was rapid and remained at almost the same level during the 90-min scan. The radioactivity in the occipital cortex was only slightly higher than that in the frontal cortex and cerebellum. Co-injection and posttreatment injection (30 min after injection of the tracer) of DAA1106 (1 mg/kg) or PK11195 (5 mg/kg) enhanced inhibition and displacement of [^11^C]DAA1106 binding by 80% and 70%, respectively. These results confirmed that these changes represented alterations in specific binding. [^11^C]DAA1106 binding (0.02% dose/ml) was three-fold higher than [^11^C]PK11195 binding (0.005% dose/ml) in the monkey occipital cortex at 30 min after injection partly because of better lipophilicity and higher affinity of [^11^C]DAA1106. The log P values for [^11^C]PK11195 and [^11^C]DAA1106 were 2.7 and 3.7, respectively. DAA1106 was reported to have a two- to three-fold higher affinity for PBR in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=DAA1106%20and%20human)]

Ikoma et al. (15) performed human PET studies using graphical analysis (GA), nonlinear least-squares (NLS) method, and multilinear analysis (MA) to evaluate the cerebral kinetics of [^11^C]DAA1106 in seven healthy subjects. Binding potential (BP) was calculated by NLS, and distribution volume (DV) was estimated by NLS, GA, and MA in various brain regions with use of a two-tissue compartmental model. DVs estimated with each method were well correlated. BP values were most reliably estimated by NLS. The highest BP value was in the thalamus (5.54), followed by the cerebellum (5.00), anterior cingulated (4.93), lateral temporal cortex (4.91), frontal cortex (4.86), parietal cortex (4.75), occipital cortex (4.70), and striatum (4.38).

## NIH Support

RO1 MH64921, K24 MH01717, K08 HD40833

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Zhang M.R., Kida T., Noguchi J., Furutsuka K., Maeda J., Suhara T., Suzuki K. (2003). [(11)C]DAA1106: radiosynthesis and in vivo binding to peripheral benzodiazepine receptors in mouse brain. Nucl Med Biol.
11 Probst K.C., Izquierdo D., Bird J.L., Brichard L., Franck D., Davies J.R., Fryer T.D., Richards H.K., Clark J.C., Davenport A.P., Weissberg P.L., Warburton E.A. (2007). Strategy for improved [(11)C]DAA1106 radiosynthesis and in vivo peripheral benzodiazepine receptor imaging using microPET, evaluation of [(11)C]DAA1106. Nucl Med Biol.
12 Maeda J., Suhara T., Zhang M.R., Okauchi T., Yasuno F., Ikoma Y., Inaji M., Nagai Y., Takano A., Obayashi S., Suzuki K. (2004). Novel peripheral benzodiazepine receptor ligand [11C]DAA1106 for PET: an imaging tool for glial cells in the brain. Synapse.
13 Venneti S., Lopresti B.J., Wang G., Slagel S.L., Mason N.S., Mathis C.A., Fischer M.L., Larsen N.J., Mortimer A.D., Hastings T.G., Smith A.D., Zigmond M.J., Suhara T., Higuchi M., Wiley C.A. (2007). A comparison of the high-affinity peripheral benzodiazepine receptor ligands DAA1106 and (R)-PK11195 in rat models of neuroinflammation: implications for PET imaging of microglial activation. J Neurochem.
14 Venneti S., Wagner A.K., Wang G., Slagel S.L., Chen X., Lopresti B.J., Mathis C.A., Wiley C.A. (2007). The high affinity peripheral benzodiazepine receptor ligand DAA1106 binds specifically to microglia in a rat model of traumatic brain injury: implications for PET imaging. Exp Neurol.
15 Ikoma Y., Yasuno F., Ito H., Suhara T., Ota M., Toyama H., Fujimura Y., Takano A., Maeda J., Zhang M.R., Nakao R., Suzuki K. (2007). Quantitative analysis for estimating binding potential of the peripheral benzodiazepine receptor with [(11)C]DAA1106. J Cereb Blood Flow Metab.